# Sialy Lewis^x^ mimetic conjugated to ultrasmall superparamagnetic iron oxide nanoparticles

Chemical name: | Sialy Lewis^x^ mimetic conjugated to ultrasmall superparamagnetic iron oxide nanoparticle
Abbreviated name: | USPIO-g-sLe^x^
Synonym:
Agent category: | Compound
Target: | E-selectin
Target category: | Receptor
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal: | Iron oxide
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=34420911), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=4506870) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=6401) for more information about E-selectin.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO%20E-selectin)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used to create images because of their abundance in water molecules. Water comprises ~80% of most soft tissue. The contrast of proton MRI depends mainly on the density of the nucleus (proton spins), the relaxation times of the nuclear magnetization (T1, longitudinal; T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the development of contrast agents. Most contrast agents affect the T1 and T2 relaxation times of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1). Cross-linked iron oxide (CLIO) nanoparticles and other iron oxide formulations affect T2 primarily and lead to decreased signals. On the other hand, the paramagnetic T1 agents, such as gadolinium (Gd^3+^), and manganese (Mn^2+^), accelerate T1 relaxation and lead to brighter contrast images.

The superparamagnetic iron oxide (SPIO) structure is composed of ferric iron (Fe^3+^) and ferrous iron (Fe^2+^). The iron oxide particles are coated with a protective layer of dextran or other polysaccharide. These particles have large combined magnetic moments or spins, which are randomly rotated in the absence of an applied magnetic field. SPIO is used mainly as a T2 contrast agent in MRI, though it can shorten both T1 and T2/T2* relaxation processes. SPIO particle uptake into the reticuloendothelial system (RES) is by endocytosis or phagocytosis. SPIO particles are also taken up by phagocytic cells such as monocytes, macrophages, and oligodendroglial cells. A variety of cells can be labeled with these particles for cell trafficking and tumor-specific imaging studies. SPIO agents are classified by their sizes with coating material (~20–3,500 nm in diameter) as large SPIO (LSPIO) nanoparticles, standard SPIO (SSPIO) nanoparticles, ultrasmall SPIO (USPIO) nanoparticles, and monocrystalline iron oxide nanoparticles (MION) (1).

USPIO is composed of iron nanoparticles of 4–6 nm diameter and the hydrodynamic diameter with dextran coating is 20–50 nm. USPIO nanoparticles have a long plasma half-life because of their small size. The blood pool half-life of plasma relaxation times is calculated to be ~24 h in humans (2) and 2 h in mice (3). Because of its long blood half-life, USPIO can be used as blood pool agent during the early phase of intravenous administration (4). In the late phase, USPIO is suitable for the evaluation of the RES in the body, particularly in lymph nodes (5).

E-selectin is found on the cell surface of endothelial cells (6, 7). It binds to sialy-Lewis^x^ (a carbohydrate moiety) on the cell-surface of leukocytes. Tumor necrosis factor α (TNFα) and interleukin-1 (IL-1), released from inflammatory stimuli, upregulate E-selectin and other adhesion molecule expression on the vascular endothelial cells, which leads to leukocyte adhesion to the activated endothelium. E-selectin and other selectins are involved in arresting leukocytes on the endothelium. A sialy-Lewis^x^ mimetic was conjugated to USPIO nanoparticles for non-invasive MRI of E-selectin expression on activated endothelial cells (8).

### Related Resource Links:

- Chapters in MICAD (E-selectin (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=E-selectin%5BAll+Fields%5D+AND+micad%5Bbook%5D))
- Gene information in NCBI (E-selectin (http://www.ncbi.nlm.nih.gov/gene/6401)).
- Articles in Online Mendelian Inheritance in Man (OMIM) (E-selectin (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=omim&Cmd=DetailsSearch&Term=E-selectin%5BAll+Fields%5D))
- Clinical trials (E-selectin (http://www.clinicaltrials.gov/ct2/results?term=E-selectin))
- Drug information in FDA (E-selectin (http://google2.fda.gov/search?q=e-selectin&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=13&y=6))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO%20E-selectin%20and%20synthesis)]

Dextran-coated USPIO nanoparticles (20–40 nm) were crosslinked with epichlorohydrin in the presence of sodium hydroxide at 40ºC for 24 h (8). A solution of sialy-Lewis^x^ mimetic (10 mg) was added to the USPIO-epichlorhydrin suspension (0.15 mmol Fe) and mixed at room temperature for 18 h. USPIO-g-sLe^x^ was purified with dialysis. USPIO-g-sLe^x^ and USPIO exhibited r_2_ values of 73 and 78.6 mM^-1^ s^-1^ at 60 MHz and 37ºC, respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO%20E-selectin%20and%20in%20vitro)]

Boutry et al. (8) performed in vitro binding studies of USPIO-g-sLe^x^ and USPIO in cultured human umbilical vein endothelial cells (HUVECs) with T2-weighted MRI. HUVECs were stimulated with TNFα and incubated with 4 mM of USPIO-g-sLe^x^ or USPIO for 1 h, which showed extensive retention of USPIO-g-sLe^x^ on TNFα-stimulated HUVECs. Image intensity and R_2_ measurements performed on T2-weighted MR images demonstrated a significantly higher (P<0.01) negative enhancement of USPIO-g-sLe^x^ than USPIO on stimulated HUVECs and on non-stimulated HUVECs.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO%20E-selectin%20and%20rodentia)]

Hepatitis was induced in NMRI mice by intravenous injection of concanavalin A. USPIO-g-sLe^x^ (n = 3 mice) and USPIO (n = 3 mice) were injected intravenously into hepatitis-positive and healthy mice (8). USPIO nanoparticles are known to be captured by Kupffer cells (liver macrophages) after passing through the fenestrae of the liver, which induces a loss of signal intensity on T2-weighted MR images. Unexpectedly, when injected in hepatitis-positive mice, USPIO-g-sLe^x^ induced a significantly lower (P <0.05–0.01) attenuation of liver signal intensity than USPIO or USPIO-g-sLe^x^ injected into healthy mice, or USPIO injected into hepatitis-positive mice at 1–2 h after contrast media injections. These data suggest that most of USPIO-g-sLe^x^ is retained extracellularly by an interaction with E-selectin overexpressed on the hepatitis-positive vascular endothelium, and therefore not captured by the liver macrophages.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO%20E-selectin%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO%20E-selectin%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=USPIO%20E-selectin%20and%20human)]

No publication is currently available.

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 McLachlan S.J., Morris M.R., Lucas M.A., Fisco R.A., Eakins M.N., Fowler D.R., Scheetz R.B., Olukotun A.Y. (1994). Phase I clinical evaluation of a new iron oxide MR contrast agent. J Magn Reson Imaging.
3 Weissleder R., Elizondo G., Wittenberg J., Rabito C.A., Bengele H.H., Josephson L. (1990). Ultrasmall superparamagnetic iron oxide: characterization of a new class of contrast agents for MR imaging. Radiology.
4 Stillman A.E., Wilke N., Li D., Haacke M., McLachlan S. (1996). Ultrasmall superparamagnetic iron oxide to enhance MRA of the renal and coronary arteries: studies in human patients. J Comput Assist Tomogr.
5 Anzai Y., Piccoli C.W., Outwater E.K., Stanford W., Bluemke D.A., Nurenberg P., Saini S., Maravilla K.R., Feldman D.E., Schmiedl U.P., Brunberg J.A., Francis I.R., Harms S.E., Som P.M., Tempany C.M. (2003). Evaluation of neck and body metastases to nodes with ferumoxtran 10-enhanced MR imaging: phase III safety and efficacy study. Radiology.
6 Bird M.I., Foster M.R., Priest R., Malhotra R. (1997). Selectins: physiological and pathophysiological roles. Biochem Soc Trans.
7 Rosen S.D., Bertozzi C.R. (1994). The selectins and their ligands. Curr Opin Cell Biol.
8 Boutry S., Laurent S., Elst L.V., Muller R.N. (2006). Specific E-selectin targeting with a superparamagnetic MRI contrast agent. Contrast Media Mol Imaging.